# ^177^Lu-Labeled DOTA-conjugated AE105 peptide (Asp-Cha-Phe-(D)Ser-(D)Arg-Tyr-Leu-Trp-Ser-CONH_2_)

Chemical name: | ^177^Lu-Labeled DOTA-conjugated AE105 peptide (Asp-Cha-Phe-(D)Ser-(D)Arg-Tyr-Leu-Trp-Ser-CONH_2_)
Abbreviated name: | [^177^Lu]-DOTA-AE105
Synonym:
Agent Category: | Peptide
Target: | Urokinase-type plasminogen activator receptor (uPAR)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Urokinase-type%20plasminogen%20activator%20receptor&cmd=DetailsSearch)]

The urokinase type plasminogen activator (uPA) receptor (uPAR) is implicated in bacterial infections, hemoglobinuria (the paroxysmal nocturnal type), and cancers such as those of the colon-rectum, stomach, and the mammary glands (1). The role and functions of uPAR in cellular physiology have been discussed in detail by Kriegbaum et al. (1).The expression of uPAR is either very low or undetectable in normal tissues, but it is overexpressed in cancerous lesions during the development of neoplastic tumors and metastasis of the disease (2). The expression levels of uPAR in cancerous tumors and the levels of soluble uPAR in the blood of cancer patients are prognostic biomarkers and can predict the outcome for an individual suffering from cancer (3). uPAR is considered an important target for the detection and treatment of colorectal cancer (CRC) because it plays an important role in tissue remodeling during the pathogenesis of this disease (1, 4). Therefore, uPAR has been targeted for the noninvasive detection of CRC with probes using different types of imaging modalities, including positron emission tomography (PET) (1, 4). A radiolabeled linear peptide that has a high affinity for the uPAR, AE105 (Asp-Cha-Phe-(D)Ser-(D)Arg-Tyr-Leu-Trp-Ser-CONH_2_), is considered to be the most promising ligand for the detection and imaging of cancerous tissues that overexpress the uPAR (1). It was demonstrated that ^64^Cu- or ^68^Ga-labeled AE105 can be used with PET to detect and visualize xenograft tumors that overexpressed uPAR in rodents (5, 6). In an effort to develop a radiolabeled peptide that can be used for the radiotherapy of CRC, the AE105 peptide was conjugated with 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid and labeled with ^177^Lu ([^177^Lu]-DOTA-AE105) (4). The biodistribution of [^177^Lu]-DOTA-AE105 was studied in nude mice bearing HT-29 cell (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology) (a human colorectal adenocarcinoma cell line that overexpresses uPAR) xenograft tumors.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=uPAR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)

Human uPAR in Gene database (http://www.ncbi.nlm.nih.gov/gene/5329); Gene ID: 5329

uPAR in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/173391))

Human uPAR protein and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/48146020) sequences

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Urokinase-type+plasminogen+activator+receptor+) related to uPAR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22739362%5Buid%5D&cmd=DetailsSearch)]

AE105 and its inactive mutant analog AE105mut (DOTA-Asp-Cha-Glu-(D)Ser-(D)Arg-Tyr-Leu-Glu-Ser-CONH_2_) were synthesized with Fmoc solid-phase peptide chemistry as described elsewhere (5). The two peptides were labeled with ^177^Lu as detailed by Persson et al. (4). The radiochemical yield (RCY) and radiochemical purity (RCP) of the labeled peptides were 60% and 95%–97%, respectively. The specific activities of the labeled peptides were not reported.

For use as controls in PET/computed tomography (CT) imaging studies, the AE105 peptide was labeled with ^64^Cu ([^64^Cu]-DOTA-AE105) (4). In an earlier study, the RCY and RCP of the ^64^Cu-labeled peptide were reported to be >90% and >95%, respectively, and the specific activity of the peptide was 25 GBq/μmol (925 mCi/μmol) (5).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22739362%5Buid%5D&cmd=DetailsSearch)]

ELISA of whole tumor extracts obtained from mice treated with [^177^Lu]-DOTA-AE105 showed significantly lower levels of uPAR (P < 0.05) compared with the uPAR levels in tumors obtained from the control group (injected with vehicle alone) or animals injected with [^177^Lu]-DOTA-AE105mut. No differences in the levels of uPAR were apparent in tumors from animals injected with the vehicle alone or the [^177^Lu]-DOTA-AE105mut peptide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu%20DOTA-AE105%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^177^Lu]-DOTA-AE105 and [^177^Lu]-DOTA-AE105mut (control) was studied in nude mice bearing HT-29 cell xenograft tumors (n = 4 animals/time point) (4). The animals were injected with 2–3 MBq (74–111 μCi) [^177^Lu]-DOTA-AE105 or [^177^Lu]-DOTA-AE105mut, and the rodents were euthanized at time points ranging from 0.5 h to 24 h postinjection (p.i.) to determine the amount of radioactivity accumulated in the organs of interest, including tumors. Results obtained from this study were presented as percent of injected dose per gram of tissues (% ID/g) (Table 1).

Table 1: Biodistribution of [ ^ 177 ^ Lu]-DOTA-AE105 and [ ^ 177 ^ Lu]-DOTA-AE105mut (control) in nude mice bearing HT-29 cell tumors ( 4 ).

Tissues | ^ 177 ^ Lu-labeled peptides
Tissues | AE105mut | AE105
Tissues | Time points (h)
Tissues | 0.5 | 0.5 | 1.0 | 2.0 | 4.0 | 24.0
Tissues | Uptake of radioactivity (% ID/g)
Blood | 0.959 | 2.709 | 0.282 | 0.173 | 0.043 | 0.006
Liver | 0.228 | 0.686 | 0.249 | 0.243 | 0.284 | 0.149
Kidney | 3.013 | 6.174 | 2.440 | 1.909 | 1.667 | 0.839
Muscle | 0.235 | 0.580 | 0.084 | 0.047 | 0.053 | 0.010
Tumor | 0.708 | 1.779 | 0.614 | 0.170 | 0.176 | 0.057
Tumor/muscle ratio | 3.01 | 3.06 | 7.30 | 3.60 | 3.32 | 5.70

For complete data, see Perssons et al. ( 4 ).

With [^177^Lu]-DOTA-AE105, maximum radioactivity was detected in the kidneys, followed by the tumors and the blood, at 0.5 h p.i. By comparison, a significantly reduced uptake of label was observed with [^177^Lu]-DOTA-AE105mut in the tumors at this time point (P < 0.05). The tumor/muscle ratios with [^177^Lu]-DOTA-AE105 were 3.06 and 7.30 at 0.5 h p.i. and 1 h p.i., respectively; these ratios subsequently decreased to 3.60 at 2 h p.i. and stayed relatively constant thereafter. No blocking studies were reported.

A single mouse was injected with 20 MBq (740 μCi) [^177^Lu]-DOTA-AE105 for gamma planar imaging at 1 h p.i. as described by Persson et al. (4). For use as a control, another mouse was injected with 10 MBq (370 μCi) [^64^Cu]-DOTA-AE105, and PET/CT images of the animals were acquired at 1 h p.i. From the PET/CT images it was clear that the label accumulated primarily in the liver and tumor tissues of the animal. The gamma planar image showed that the probe was taken up primarily by the kidneys, liver, and the tumors. However, the tumors were visible more clearly in the PET images than in the gamma planar images. A manual region-of-interest analysis of the PET and the gamma planar images showed that uptake of the tracer by the tumors was 0.86 ± 0.03% ID/g and 0.61 ± 0.15% ID/g with [^64^Cu]-DOTA-AE105 and [^177^Lu]-DOTA-AE105, respectively. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu%20DOTA-AE105%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu%20DOTA-AE105%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22739362%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kriegbaum M.C., Persson M., Haldager L., Alpizar-Alpizar W., Jacobsen B., Gardsvoll H., Kjaer A., Ploug M. (2011). Rational targeting of the urokinase receptor (uPAR): development of antagonists and non-invasive imaging probes. Curr Drug Targets.
2 Nielsen B.S., Rank F., Illemann M., Lund L.R., Dano K. (2007). Stromal cells associated with early invasive foci in human mammary ductal carcinoma in situ coexpress urokinase and urokinase receptor. Int J Cancer.
3 Rasch M.G., Lund I.K., Almasi C.E., Hoyer-Hansen G. (2008). Intact and cleaved uPAR forms: diagnostic and prognostic value in cancer. Front Biosci.
4 Persson, M., P. Rasmussen, J. Madsen, M. Ploug, and A. Kjaer, New peptide receptor radionuclide therapy of invasive cancer cells: in vivo studies using (177)Lu-DOTA-AE105 targeting uPAR in human colorectal cancer xenografts. Nucl Med Biol, 2012
5 Persson M., Madsen J., Ostergaard S., Jensen M.M., Jorgensen J.T., Juhl K., Lehmann C., Ploug M., Kjaer A. (2012). Quantitative PET of human urokinase-type plasminogen activator receptor with 64Cu-DOTA-AE105: implications for visualizing cancer invasion. J Nucl Med.
6 Persson M., Madsen J., Ostergaard S., Ploug M., Kjaer A. (2012). 68Ga-labeling and in vivo evaluation of a uPAR binding DOTA- and NODAGA-conjugated peptide for PET imaging of invasive cancers. Nucl Med Biol.